# 3-(3-(3-[^18^F]Flouropropyl)thio)-1,2,5-thiadiazol-4-yl)-1,2,5,6-tetrahydro-1-methylpyridine

Chemical name: | 3-(3-(3-[^18^F]Flouropropyl)thio)-1,2,5-thiadiazol-4-yl)-1,2,5,6-tetrahydro-1-methylpyridine
Abbreviated name: | [^18^F]FP-TZTP
Synonym:
Backbone: | Compound
Target: | Muscarinic M_2_ receptor
Mechanism: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FP-TZTP)]

The current state of molecular genetics of Alzheimer’s disease (AD) focuses on four genes: the β-amyloid precursor protein (β-APP) gene, the presenilin 1 gene, the presenilin 2 gene, and the apolipoprotein E (APOE) gene (2). The ε4 allele of the APOE gene is associated with an increased risk for late-onset AD (>50 years of age). Few of the imaging studies to date have been based on these genetic abnormalities. The characteristic neuropathology is neurofibrillary tangles and amyloid plaques. The result of the phenotypic changes is caused by an alteration in the processing of β-APP favoring the production of the potentially toxic Aβ42 protein. Binding of radioligands to Aβ42 protein in vivo has been reported (3). There has also been a report on the use of 2-[^18^F]fluoro-2-deoxyglucose ([^18^F]FDG) in a subpopulation of AD patients with the APOE gene (4), although this is an indirect measure of the phenotype. The authors found changes in FDG distribution before clinical manifestations.

Muscarinic cholinergic M_2_ subtype-selective ligands were developed based on the observation that this subtype is lost in the cerebral cortex in AD (5-7). Postmortem quantization of muscarinic subtypes indicated a selective loss of the M_2_ subtype in cortical regions, whereas the M_1_ subtype was preserved. Thus, an M_2_-selective ligand labeled with a positron-emitting radionuclide would allow determination of M_2_ subtype density in the living human brain. Several investigators have pursued muscarinic receptor imaging with positron emission tomography (2) and single-photon emission computed tomography (SPECT) (8, 9). Most tracers for cholinergic receptors have not demonstrated subtype selectivity. Alternatively, ligands that are subtype selective in vitro typically do not cross the blood-brain barrier (BBB). In addition to muscarinic receptors, ligands for the nicotinic receptors (10, 11) and acetylcholinesterase (12) have been investigated. Acetylcholinesterase (13-15) has been a target for radioligand development because its levels also change in AD. In addition, the vesicular acetylcholine (ACh) transporter has been studied recently in patients with AD using [^123^I]iodobenzovesamicol (12). The probe for acetylcholinesterase (N-[^11^C]methylpiperdin-4-yl propionate, [^11^C]PMP) has been used in AD patients and found to show a decrease that is more uniform and broadly distributed than the focal defects found with [^18^F]FDG (12). 3-((3-(3-fluoropropyl)thio)-1,2,5-thiadiazol-4-yl)-1,2,5,6-tetrahydro-1-methylpyridine (FP-TZTP), a muscarinic agonist based on a series of non-fluorinated analogs first proposed by Sauerberg et al. (16), was radiolabeled with the positron-emitting radionuclide ^18^F ([^18^F]FP-TZTP) (17). [^18^F]FP-TZTP was found to be a promising imaging agent for the M2 system in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FP-TZTP%20and%20synthesis)]

Nucleophilic fluorination of (3-(3-((3-(methanesulfonyoxy)-propyl)thio)-1,2,5-thiadiazol-4-yl)-1,2,5,6-tetrahydro-1-methylpyridine with K[^18^F]F/Kryptofix2.2.2 to form [^18^F]FP-TZTP (18). A one-step radiosynthesis of [^18^F]FP-TZTP was developed and can also be conducted with an automated synthesis unit. The manual synthesis produced [^18^F]FP-TZTP in a radiochemical yield of 23.4% ± 4.3% (EOS, n = 69) with a specific activity of 117 ± 54 MBq/μmol, 4377 ± 2011 mCi/μmol (EOB, n = 100). The automated synthesis unit provided [^18^F]FP-TZTP in a radiochemical yield of 18.8% ± 2.4% (EOS, n = 25) with a specific activity of 111 ± 70 MBq/μmol, 4112 ± 2572 mCi/μmol (EOB, n = 25) (18).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FP-TZTP%20and%20in%20vitro)]

FP-TZTP showed a K_i_ of 7.4 nM for M_1_ and 2.2 nM for M_2_. It did not bind to M_3_ receptors or other biogenic amine receptors (19).

Rat hepatocytes were incubated with [^18^F]FP-TZTP with (carrier-added) or without (no-carrier-added) the addition of 20 μg of unlabeled FP-TZTP. The time course of metabolites from the sequential analysis of the no-carrier-added experiment revealed that the parent compound was nearly consumed within 2 h, concomitant with the formation of seven radiolabeled metabolites. The carrier-added experiment showed slower metabolism. The 30-min, carrier-added sample was selected for identification of the metabolites by liquid chromatography tandem mass spectrometry (LC/MS/MS). Structures were confirmed for all compounds by comparison of retention time and MS/MS fragmentation with the synthesized standards. N-Oxidation provided the major radioactive metabolite. Other major metabolites were formed from sulfur oxidation, demethylation of the tertiary amine, and dehydrogenation of the tetrahydropyridine ring, respectively. In addition to the major metabolites of FP-TZTP identified above, two more polar radioactivity peaks were found in the radiochromatogram. The peak eluting at the solvent front was identified as [^18^F]fluoride. The remaining peak was unidentified based on the MS/MS data. Compared with rat hepatocytes, human hepatocytes produced a similar metabolite profile. The N-oxide was also the major metabolite identified by LC/MS and radiochromatography. However, N-oxidation metabolites were not obtained with the same dominance as observed in rat hepatocytes. Demethylation and S-oxidation metabolites were also produced by human hepatocytes. The ring oxidation metabolite and its hydroxylated analog were also found in human hepatocytes (20).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FP-TZTP%20and%20rodentia)]

Metabolism of [^18^F]FP-TZTP in vivo is rapid (21). In rat, only 5% of plasma radioactivity was in the parent compound by 15 min after injection. One metabolite was almost as lipophilic as the parent compound, as measured by TLC, suggesting that it might cross the BBB. However, the parent compound was found to represent >95% of extracted radioactivity in rat brain through 30 min and >90% at 45 and 60 min.

Autoradiography using no-carrier-added [^18^F]FP-TZTP confirmed the uniform distribution of radioactivity characteristic of the M_2_ pattern of localization (22). Coinjection of a muscarinic agonist, (3-(propylthio)-l,2,5-thiadiazol-4-yl)-tetrahydro-l-methyl-pyridine (P-TZTP), at 5, 50, and 500 nmol inhibited [^18^F]FP-TZTP uptake in a dose-dependent manner at 1 hour after i.v. injection. The difference in brain regions between each dose level was significant (p < 0.01), except for the 5-nmol value in the medulla (p < 0.06). The brain distribution of the agonist [^18^F]FP-TZTP was unaffected by coinjection of 5, 50, or 500 nmol of the antagonist R-3-quinuclidinyl-R-4-[^123^I]iodobenzilate (RR-IQNB). Likewise, the distribution of [^18^F]FP-TZTP was unaffected by co-injection of 500 nmol of the M_2_-selective antagonist RS-FMeQNB except in the cerebral cortex and hippocampus, where the difference was significant (p < 0.03). Binding in the heart was low by 15 min; therefore, earlier time points were studied. At 5 min, 55% inhibition of uptake in the heart was observed with co-injection of P-TZTP.

Biodistribution of [^18^F]FP-TZTP was studied in WT mice and in genetically engineered mice lacking functional M_1_, M_2_, M_3_, or M_4_ muscarinic receptors (23). Using ex vivo autoradiography, the regional brain localization of [^18^F]FP-TZTP in M_2_ knockout (M_2_ KO) mice was significantly decreased (51.3% to 61.4%; p < 0.01) compared with the WT mice in amygdala, brain stem, caudate putamen, cerebellum, cortex, hippocampus, hypothalamus, superior colliculus, and thalamus. In similar studies with M_1_ KO, M_3_ KO, and M_4_ KO mice compared with WT mice, [^18^F]FP-TZTP uptake in the same brain regions was not significantly decreased. [^18^F]FP-TZTP preferentially labels M_2_ receptors in vivo because large decreases in [^18^F]FP-TZTP brain uptake were seen only in M_2_ KO versus WT mice,.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FP-TZTP%20and%20(dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FP-TZTP%20and%20primate%20not%20human)]

PET studies of isoflurane-anesthetized rhesus monkeys were performed to assess the in vivo behavior of [^18^F]FP-TZTP (24). Control studies were performed to characterize tracer kinetics and to choose an appropriate mathematical model for the in vivo behavior of the tracer. Metabolite correction of the arterial input data was performed using TLC. The parent compound represented 48 ± 9%, 28 ± 6%, and 13 ± 3% plasma radioactivity at 15, 30, and 90 min, respectively. [^18^F]FP-TZTP time-activity curves in brain were well described by a one-compartment model with three parameters: uptake rate constant K1, total volume of distribution V and a global brain-to-blood time delay Δt. Tracer uptake in the brain was rapid, with K1 values of 0.4 to 0.6 ml/min/ml in gray matter.

The volume of distribution V represents total tracer binding (free, nonspecifically bound, and specifically bound). V values were similar (22-26 ml/ml) in cortical regions, basal ganglia, and thalamus but were significantly lower (16 ml/ml, p < 0.01) in the cerebellum. In comparing these V values with the receptor distribution reported for rat and monkey, there was an excellent match with the M_2_ distribution. In rat, the concentrations of M_2_ receptors in cortical structures, basal ganglia, and thalamus are highly uniform and are approximately 50% lower in cerebellum (25). In rhesus monkey, the distributions of M_2_ receptors are also uniform in cortex, basal ganglia, and thalamus (26). This pattern is unlike that of M_1_ receptors (the muscarinic subtype to which this tracer shows threefold lower in vitro affinity) for which basal ganglia > cortex > thalamus (26, 27).

Preblocking studies were used to measure nonspecific binding. Pre-administering 200-400 nmol/kg of nonradioactive FP-TZTP produced a dramatic reduction in total binding of about 50% in cerebellum and 60-70% in other gray matter regions. Similar blockade was seen in analogous rat studies (19). This reduction was highly significant in all regions, and the regional distribution of V values after pre-blocking became nearly uniform. In addition to preblocking studies, displacement of [^18^F]FP-TZTP with 80 nmol/kg of FP-TZTP at 45 min after injection caused a distinct increase in net efflux with decreases of 20%, 36%, and 41% in cerebellum, cortex, and thalamus, respectively (21). The sensitivity of [^18^F]FP-TZTP binding to changes in brain ACh was assessed by administering physostigmine, an acetylcholinesterase inhibitor, by i.v. infusion beginning 30 min before tracer injection. Physostigmine produced a 35% reduction in cortical-specific binding (p < 0.05), consistent with increased competition from ACh.

[^18^F]FP-TZTP was used to assess the muscarinic effects of procaine (28), which has been used previously to induce emotional and psychosensory experiences in healthy controls and patients with mood disorders (29). With paired monkey studies on the same day using continuous infusion of procaine (0.016-0.5 mg/kg/min), [^18^F]FP-TZTP-specific binding was globally blocked up to 90% in a dose-dependent manner with an EC_50_ of about 0.063 mg/kg/min. This suggested a role for M_2_ receptors in procaine-induced effects in consistent with a cholinergic hypothesis of mood regulation.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FP-TZTP%20and%20human)]

[^18^F]FP-TZTP dosimetry in humans was determined from its biodistribution in monkeys by i.v. of 93-130 MBq (2.5-3.5 mCi) [^18^F]FP-TZTP (30). There was early accumulation of activity in liver and kidney, with subsequent appearance of activity in gallbladder and urine, reflecting pathways for tracer excretion. The effective dose equivalent was 0.023 mSv/MBq (85 mrem/mCi). The critical organ was urinary bladder (0.073 mGy/MBq, 269 mrad/mCi), followed by pancreas (0.047 mGy/MBq, 173 mrad/mCi), gallbladder (0.040 mGy/MBq, 147 mrad/mCi), and brain (0.023 mGy/MBq, 86 mrad/mCi).

[^18^F]FP-TZTP PET was studied in healthy volunteers (31). In plasma, the parent compound represented 68 ± 8%, 41 ± 9%, and 14 ± 4% of radioactivity at 20, 40, and 120 min, respectively. The plasma-free fraction was 5.9 ± 1.2%. A model with one tissue compartment produced an excellent fit for the full 120 min of data, so that the additional parameters of a two-compartment model were unidentifiable. K1 values in gray matter regions were high, 0.36 to 0.56 ml/min/ml, and showed excellent correlation with cerebral blood flow. V values, representing total tissue binding, were similar in cortical regions, basal ganglia, and thalamus but were significantly higher (p < 0.01) in amygdala. Unlike the results in the monkey, binding in the cerebellum was similar to that in the cerebral cortex.

In the first clinical studies, an age-related increase in M_2_ receptor binding potential was observed using [^18^F]FP-TZTP and PET in normal subjects (32). There was a significant increase not only in the average volume of distribution but also for variance in the older subjects. This infers that other aspects of the systems biology were coming into play, and therefore the data should be modeled by a more complex set of equations. The increase in variance for the volume of distribution was caused by using age discrimination only. This suggested the possibility that the age-related changes might be associated with a specific genotype, such as the APOE-ε4 allele. In the following study, Cohen et al. (33) found that the gray matter distribution volume for [^18^F]FP-TZTP was significantly higher in the APOE-ε4-positive normal subjects than in the APOE-ε4-negative normal subjects, whereas there were no differences in global cerebral blood flow. Given that [^18^F]FP-TZTP measures the muscarinic system rather than only receptor density because of its agonist properties, changes in receptor binding affinity attributable to changes in G protein binding and competition with ACh at the muscarinic receptor can be monitored. The increased volume of distribution in elderly normal subjects with APOE-ε4 positivity may be because of a decreased concentration of ACh in the synapse, which would lead to higher binding of [^18^F]FP-TZTP. This type of competition was shown to be possible in the studies in monkeys using physostigmine (21). As a result, the use of [^18^F]FP-TZTP can be considered an in vivo measurement of muscarinic systems biology, rather than of receptor density alone.

## Supplemental Information

[Disclaimers (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=disclaimer)]

Synthesis Protocol A

Synthesis Protocol B

Preclinical Pharmacology

## NIH Support

Intramural Research Program

## References

1 Slavicek J.M., Hayes-Plazolles N. (2003). The Lymantria dispar nucleopolyhedrovirus contains the capsid-associated p24 protein gene. Virus Genes.
2 St George-Hyslop P.H., Petit A. (2005). Molecular biology and genetics of Alzheimer's disease. C R Biol.
3 Bacskai B.J., et al. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
4 Frey K.A., Minoshima S., Kuhl D.E. (1998). Neurochemical imaging of Alzheimer's disease and other degenerative dementias. Q J Nucl Med.
5 Aubert I., et al. (1992). Comparative alterations of nicotinic and muscarinic binding sites in Alzheimer's and Parkinson's diseases. J Neurochem.
6 Quirion R., et al. (1989). Muscarinic receptor subtypes in human neurodegenerative disorders: focus on Alzheimer's disease. Trends Pharmacol Sci.
7 Rodriguez-Puertas R., et al. (1997). Autoradiographic distribution of M1, M2, M3, and M4 muscarinic receptor subtypes in Alzheimer's disease. Synapse.
8 Freo U., et al. (2002). A short review of cognitive and functional neuroimaging studies of cholinergic drugs: implications for therapeutic potentials. J Neural Transm.
9 Maziere M. (1995). Cholinergic neurotransmission studied in vivo using positron emission tomography or single photon emission computerized tomography. Pharmacol Ther.
10 Gatley S.J., et al. (1998). In vitro and ex vivo autoradiographic studies of nicotinic acetylcholine receptors using [18F]fluoronochloroepibatidine in rodent and human brain. Nucl Med Biol.
11 Horti A.G., et al. (1998). 2-[18F]Fluoro-A-85380, an in vivo tracer for the nicotinic acetylcholine receptors. Nucl Med Biol.
12 Kuhl D.E., et al. (1999). In vivo mapping of cerebral acetylcholinesterase activity in aging and Alzheimer's disease. Neurology.
13 Kilbourn M.R., et al. (1996). In vivo studies of acetylcholinesterase activity using a labeled substrate, N-[11C]methylpiperdin-4-yl propionate ([11C]PMP). Synapse.
14 Namba H., et al. (1994). In vivo measurement of acetylcholinesterase activity in the brain with a radioactive acetylcholine analog. Brain Res.
15 Tavitian B., et al. (1993). In vivo visualization of acetylcholinesterase with positron emission tomography. Neuroreport.
16 Sauerberg P., et al. (1992). Novel functional M1 selective muscarinic agonists. Synthesis and structure-activity relationships of 3-(1,2,5-thiadiazolyl)-1,2,5,6-tetrahydro-1-methylpyridines. J Med Chem.
17 Eckelman W.C. (2001). Radiolabeled muscarinic radioligands for in vivo studies. Nucl Med Biol.
18 Kiesewetter D.O., Vuong B.K., Channing M.A. (2003). The automated radiosynthesis of [18F]FP-TZTP. Nucl Med Biol.
19 Kiesewetter D.O., et al. (1995). Preparation of 18F-labeled muscarinic agonist with M2 selectivity. J Med Chem.
20 Ma Y., et al. (2002). Identification of metabolites of fluorine-18-labeled M2 muscarinic receptor agonist, 3-(3-[(3-fluoropropyl)thio]-1,2,5-thiadiazol-4-yl)-1,2,5,6-tetrahydro-1-me thylpyridine, produced by human and rat hepatocytes. J Chromatogr B Analyt Technol Biomed Life Sci.
21 Kiesewetter D.O., et al. (1999). In vivo muscarinic binding of 3-(alkylthio)-3-thiadiazolyl tetrahydropyridines. Synapse.
22 Kiesewetter D.O., et al. (1999). Using single photon emission tomography (SPECT) and positron emission tomography (PET) to trace the distribution of muscarinic acetylcholine receptor (MACHR) binding radioligands. Life Sci.
23 Jagoda E.M., et al. (2003). Regional brain uptake of the muscarinic ligand, [18F]FP-TZTP, is greatly decreased in M2 receptor knockout mice but not in M1, M3 and M4 receptor knockout mice. Neuropharmacology.
24 Carson R.E., et al. (1998). Muscarinic cholinergic receptor measurements with [18F]FP-TZTP: control and competition studies. J Cereb Blood Flow Metab.
25 Li M., et al. (1991). Distribution of m2 muscarinic receptors in rat brain using antisera selective for m2 receptors. Mol Pharmacol.
26 Flynn D.D., Mash D.C. (1993). Distinct kinetic binding properties of N-[3H]-methylscopolamine afford differential labeling and localization of M1, M2, and M3 muscarinic receptor subtypes in primate brain. Synapse.
27 Wall S.J., et al. (1991). Production of antisera selective for m1 muscarinic receptors using fusion proteins: distribution of m1 receptors in rat brain. Mol Pharmacol.
28 Benson B.E., et al. (2004). A potential cholinergic mechanism of procaine's limbic activation. Neuropsychopharmacology.
29 Ketter T.A., et al. (1996). Anterior paralimbic mediation of procaine-induced emotional and psychosensory experiences. Arch Gen Psychiatry.
30 Herscovitch P., Kiesewetter D.O., Carson R.E. (1998). Biodistribution and radiation dose estimates for [F-18] fluoropropyl-TZTP, a new muscarinic cholinergic ligand. . J Nucl Med.
31 Carson R.E., et al. (1998). Evaluation of a new F-18 labeled analog of the 5-HT1A antagonist WAY 100635 for PET. J Nucl Med.
32 Podruchny T.A., et al. (2003). In vivo muscarinic 2 receptor imaging in cognitively normal young and older volunteers. Synapse.
33 Cohen R.M., et al. (2003). Higher in vivo muscarinic-2 receptor distribution volumes in aging subjects with an apolipoprotein E-epsilon4 allele. Synapse.